# IRDye800-2-(3-{5-[7-(5-amino-1-carboxy-pentylcarbamoyl)-heptanoylamino]-1-carboxy-pentyl}-ureido)-pentanedioic acid

Chemical name: | IRDye800-2-(3-{5-[7-(5-amino-1-carboxy-pentylcarbamoyl)-heptanoylamino]-1-carboxy-pentyl}-ureido)-pentanedioic acid
Abbreviated name: | YC-27
Synonym:
Agent category: | Compound
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Antigen
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-4). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–650 nm) are used. Near-infrared (NIR) fluorescence (650–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals (4, 5).

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (6, 7). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (7). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (8). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (9). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (7). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although a commercially available monoclonal antibody (^111^In-labeled Capromomab pendetide (^111^In-CYT-356)) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (10). In addition, this antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (11, 12). 2-(3-{5-[7-(5-Amino-1-carboxy-pentylcarbamoyl)-heptanoylamino]-1-carboxy-pentyl}-ureido)-pentanedioic acid (compound 2) was conjugated with IRDye800CW to form IRDye800CW-2 (YC-27) (13), which is an inhibitor of NAALADase. YC-27 has been studied for use as an NIR agent for imaging PSMA expression in nude mice bearing human cancer xenografts.

### Related Resource Links:

- Chapters in MICAD (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PSMA+AND+micad%5Bbook%5D))
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2346))
- Articles in OMIM Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=602640))
- Clinical trials (PSMA (http://www.clinicaltrials.gov/ct2/results?term=PSMA))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20AND%20synthesis)]

To a solution of 430 nmol compound 2 in dimethyl sulfoxide was added 0.0114 mM N,N-diisopropylethylamine, followed by N-hydroxysuccininide ester of IRDye800CW (13). The mixture was incubated at room temperature for 2 h. YC-27 was purified with high-performance liquid chromatography. The molecular weight of YC-27 (1.59 kDa) was confirmed with mass spectroscopy. YC-27 exhibited an absorbance maximum at 774 nm and an emission maximum at 792 nm with an extinction coefficient of 158,900 M^-1^ and a fluorescence quantum yield of 0.053 in aqueous solution.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20AND%20in%20vitro)]

The binding affinity of YC-27 for PSMA was determined with the use of a NAALADase assay (13). YC-27 exhibited an inhibition constant (K_i_) value of 0.37 nM. The K_i_ value of the known urea-based NAAG peptidase inhibitor ZJ-43 was 2.1 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20and%20rodentia)]

Chen et al. (13) performed NIR fluorescence imaging studies of YC-27 (10 nmol) in nude mice (n = 3) bearing PSMA-positive PC3-PIP tumor xenografts and PSMA-negative PC3-flu tumor xenografts. The PC3-PIP tumors were clearly visualized at 18 h and up to 70.5 h after injection. On the other hand, the NIR signal from the PC3-flu tumors was weak. The PC3-PIP/PC3-flu ratio was 10 at 70.5 h. Moderate NIR fluorescence was visualized in the kidneys. Co-injection of 1 nmol YC-27 with 1,000 nmol DClBzL (PSMA inhibitor) in mice bearing the two tumors inhibited the NIR fluorescence in the PC3-PIP tumors and kidneys nearly to the background level of the PC3-flu tumors at 20.5 h after injection. The PC3-PIP/PC3-flu ratio was 26 at 20.5 h. The NIR signals in the tumors and kidneys were also confirmed with ex vivo imaging.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20AND%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=YC-27%20AND%20human)]

No publication is currently available.

## NIH Support

U24 CA92871, R01 CA134675

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Leung K., Chopra A., Shan L., Eckelman W.C., Menkens A.E. (2012). Essential parameters to consider for the characterization of optical imaging probes. Nanomedicine (Lond).
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
7 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
8 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
9 O'Keefe D.S., Uchida A., Bacich D.J., Watt F.B., Martorana A., Molloy P.L., Heston W.D. (2000). Prostate-specific suicide gene therapy using the prostate-specific membrane antigen promoter and enhancer. Prostate.
10 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
11 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
12 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
13 Chen Y., Dhara S., Banerjee S.R., Byun Y., Pullambhatla M., Mease R.C., Pomper M.G. (2009). A low molecular weight PSMA-based fluorescent imaging agent for cancer. Biochem Biophys Res Commun.